# Polyethylene glycol-gold nanoparticles

Chemical name: | Polyethylene glycol-gold nanoparticles
Abbreviated name: | PEG-AuNPs
Synonym:
Agent Category: | Metal
Target: | Phagocytes and tumor cells
Target Category: | Phagocytosis, blood pool retention
Method of detection: | X-ray, computed tomography (CT)
Source of signal: | Au
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanoparticles)]

X-Ray imaging, or computed tomography (CT), visualizes tissue density differences that provide the image contrast produced by X-ray attenuation between soft tissues and electron-dense bone (1). Radiopaque X-ray contrast agents are needed to enhance the degree of contrast between diseased tissues and normal tissues. Water-soluble X-ray contrast agents are generally based on small tri-iodobenzene compounds such as monomers or dimers (2), which can be ionic (high osmolality) or nonionic (low osmolality). When injected intravenously, commonly via intra-arterial catheterization, these agents exhibit highly nonspecific vascular permeation and rapid renal excretion, which limits their targeting performance.

Gold has not been used as an X-ray contrast agent in vivo. Gold has a higher atomic number and a higher absorption coefficient than iodine, providing 2.7-fold greater contrast/weight than iodine (3). Furthermore, imaging gold at 80–100 keV reduces interference from bone absorption and provides lower soft tissue absorption, which would reduce radiation to patients. Hainfeld et al. (3) used gold nanoparticles (AuNPs; 1.9 nm in diameter, ~50 kDa) as a CT contrast agent in mice; these experiments showed enhanced CT contrast of the vasculature, kidneys, and tumor in mice. However, plasma proteins in blood adsorb onto the surface of bare AuNPs, which produces large aggregates (4) that may result in altered pharmacokinetics and biodistribution of AuNPs (5). Polyethylene glycol (PEG) is found to minimize nonspecific adsorption of proteins onto NPs and to reduce their uptake by the liver (5). PEG-AuNPs are being studied as cancer CT imaging and photothermal agents (6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanoparticles%20X-ray%20contrast)]

Cai et al. (6) prepared AuNPs by the citrate reduction of chloroauric acid. First, 500 ml of 0.254 mM chloroauric acid was heated to 100°C. Then 17.5 ml of 1% citric acid was added to the solution to produce AuNPs. AuNPs were incubated with methoxy PEG sulfhydryl solution at room temperature for 12 h. PEG-AuNPs were ~38 nm in diameter as measured with transmission electron microscopy (TEM) images and dynamic light-scattering experiments.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanoparticles%20X-ray%20contrast%20and%20in%20vitro)]

Chithrani et al. (7) showed that AuNPs between 14 and 74 nm in diameter entered cultured HeLa tumor cells in medium containing 10% serum and were shown with TEM to be trapped in vesicles in the cytoplasm. The cellular uptake of the AuNPs increased for the first 2 h and gradually reached a plateau at 4–7 h. The uptake half-life was 2.10, 1.90, and 2.24 h at a rate of 622, 1,294, and 417 NPs/h for NPs 14, 50, and 74 nm in diameter, respectively.

Cai et al. (6) performed in vitro cytotoxicity assays in human WI-38 embryonic, human HepG2 hepatoma, and mouse macrophage RAW 264.7 cell lines. PEG-AuNPs (1.25–40 mM) showed little effect on cell viability after 24 h at 37°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanoparticles%20X-ray%20contrast%20and%20rodentia)]

Cai et al. (6) performed biodistribution studies of PEG-AuNPs (2.5 μmol Au/g PEG-AuNPs) administered to normal mice via intravenous injection. The plasma half-life of PEG-AuNPs was 14.8 ± 3.3 h. The tissue with the highest AuNP accumulation was the liver (64.4% injected dose (ID)) at 3 d, followed by the spleen (9.7% ID), small intestine (4.3% ID), lymph nodes (1.9% ID), large intestines (1.6% ID), muscle (1.3% ID), and kidneys (~1% ID). There was minimum accumulation in the brain, heart, and lung. PEG-AuNPs were taken up by the reticuloendothelial system and by phagocytes in the liver, spleen, lymph nodes, and bone marrow as measured with optical microscopy of the tissues and cells. TEM images of the liver Kupffer cells showed intracellular accumulation of NPs in the cytoplasm. The mice showed normal hematology and blood chemistry at days 3 and 14. Histological examination of nine major organs and tissues 3 days after injection showed no evidence of inflammatory cell infiltration, cell swelling, or tissue necrosis in any mice. No signs of sickness were observed in the mice up to 6 months. CT imaging of mice bearing HT-1080 fibrosarcoma tumors showed good contrast enhancement in the right ventricle (~2-fold), inferior vena cava (~2-fold), spleen (~2-fold), liver (<1-fold), and kidney (<0.5-fold) from 0.1 h up to 24 h. There was a gradual accumulation of NPs in the liver up to 3 h, which then stayed almost constant up to 72 h, whereas there was a continuous accumulation in the spleen even after 48 h. All major blood vessels were well visualized as well as vessels leading to the tumor; contrast returned to background levels by 72 h.

Kim et al. (8) performed CT imaging in rats bearing a hepatoma tumor in the liver after intravenous injection of 40 mg PEG-AuNPs (31 nm in diameter). Good contrast enhancement (~2-fold) was observed in the hepatoma versus the surrounding normal liver from 5 min to 24 h after injection. The heart and major vessels were clearly visualized for at least 4 h. There was a gradual accumulation of NPs by the liver for up to 2 h, whereas there was a continuous accumulation in the spleen even after 24 h.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanoparticles%20X-ray%20contrast%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanoparticles%20X-ray%20contrast%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanoparticles%20X-ray%20contrast%20and%20human)]

No publication is currently available.

## References

1 Yu S.B., Watson A.D. (1999). Metal-Based X-ray Contrast Media. Chem Rev.
2 Wallingford V.H. (1953). The development of organic iodine compounds as x-ray contrast media. J Am Pharm Assoc Am Pharm Assoc (Baltim).
3 Hainfeld J.F., Slatkin D.N., Focella T.M., Smilowitz H.M. (2006). Gold nanoparticles: a new X-ray contrast agent. Br J Radiol.
4 Zhang F., Skoda M.W., Jacobs R.M., Zorn S., Martin R.A., Martin C.M., Clark G.F., Goerigk G., Schreiber F. (2007). Gold nanoparticles decorated with oligo(ethylene glycol) thiols: protein resistance and colloidal stability. J Phys Chem A.
5 Otsuka H., Nagasaki Y., Kataoka K. (2003). PEGylated nanoparticles for biological and pharmaceutical applications. Adv Drug Deliv Rev.
6 Cai Q.Y., Kim S.H., Choi K.S., Kim S.Y., Byun S.J., Kim K.W., Park S.H., Juhng S.K., Yoon K.H. (2007). Colloidal gold nanoparticles as a blood-pool contrast agent for X-ray computed tomography in mice. Invest Radiol.
7 Chithrani B.D., Ghazani A.A., Chan W.C. (2006). Determining the size and shape dependence of gold nanoparticle uptake into mammalian cells. Nano Lett.
8 Kim D., Park S., Lee J.H., Jeong Y.Y., Jon S. (2007). Antibiofouling polymer-coated gold nanoparticles as a contrast agent for in vivo X-ray computed tomography imaging. J Am Chem Soc.